# IPLVVPLGGSC(Cy5.5-Cross-linked iron oxide)K(Fitc)

Chemical name: | IPLVVPLGGSC(Cy5.5-Cross-linked iron oxide)K(Fitc)
Abbreviated name: | IPL-NP
Synonym:
Agent Category: | Peptide
Target: | Hepsin
Target Category: | Enzyme binding
Method of detection: | Optical, near-infrared fluorescence,
Source of signal\contrast: | Cy5.5, iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hepsin%20and%20nanoparticle)]

Optical fluorescence imaging is increasingly used to understand biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (3). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (4). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (5).

Hepsin is a type II transmembrane serine protease that is generally not detectable in normal and benign hypertrophic prostate glands. Hepsin is also expressed in the liver, kidney, and thyroid (6). Elevated levels of hepsin have been found in prostate tumors (7). Hepsin promotes prostate cancer progression and metastasis (8). The peptide IPLVVPL was found to bind selectively to hepsin from phage library screening. Kelly et al. (9) used this sequence with linking residues GGSCK(Fitc) with Cy5.5-cross-linked iron oxide nanoparticles (Cy5.5-CLIO) to attach to the IPLVVPL to form fluorescence nanoparticles, IPLVVPLGGSC(Cy5.5-CLIO)K(Fitc). Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. IPLVVPLGGSC(Cy5.5-CLIO)K(Fitc) is being developed for NIR fluorescence imaging of hepsin expression in prostate cancer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hepsin%20and%20nanoparticle+synthesis)]

Aminated Cy5.5-CLIO was incubated with excess succinimidyl iodoacetic acid for 15 min (9). IPLVVPLGGSCK(Fitc) was coupled to the activated CLIO via a thiol-specific reaction at the C-terminal amino acid (C) for 1 h. The resulting IPLVVPLGGSC(Cy5.5-CLIO)K(Fitc) (IPL-NP) was purified with column chromatography. Each CLIO backbone contained an average of 11 peptides.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hepsin%20nanoparticle%20and+in+vitro)]

Kelly et al. (9) performed cell-binding assays (analyzed with flow cytometry and fluorescence microscopy) with IPL molecules using prostate cancer cell lines expressing hepsin (HPN-PC3 and LNCaP) as well as prostate cancer cell lines that do not express hepsin (PC3 and DU145). IPLVVPL-Fitc and IPLVVPLGGSCK(Fitc) exhibited good binding to HPN-PC3 and LNCaP cells with minimal binding to PC3 and DU145 cells. IPLVVPL inhibited IPLVVPLGGSCK(Fitc) binding to HPN-PC3 cells with a 50% inhibition constant of 1.4 ± 1.7 µM and a dissociation constant of 190 ± 2.2 nM. IPL-NP exhibited a 10-fold greater fluorescence intensity than IPLVVPLGGSCK(Fitc) in binding to HPN-PC3 cells and a >80-fold increase in fluorescence intensity in binding to NPN-PC3 cells as compared with PC3 cells. In situ fluorescent histochemical analysis of frozen human tissue samples of six normal prostate and five prostate cancers revealed that IPLVVPLGGSCK(Fitc) and IPL-NP stained 100% of the tumor cores (localized to tumor cells) and 0% of the control prostate cores.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hepsin%20and%20nanoparticle+rodentia)]

Kelly et al. (9) performed in vivo IPL-NP fluorescence-mediated tomography imaging of mice bearing an LNCaP tumor on the right flank and a PC3 tumor on the left flank. Increased fluorescence signal could be detected in the LNCaP tumor (65 ± 3 nM) 24 h after injection of 20 mg Fe/kg, whereas the PC3 tumor showed a lower signal (23 ± 1 nM) at the same time point. The blood half-life of IPL-NP was determined to be 7.4 h. Control non-conjugated nanoparticle accumulation in both tumors was ~20 nM. LNCaP tumors as small as 4.6 mm in diameter could be detected. No blocking or co-localization experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hepsin%20and%20nanoparticle%20(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hepsin%20and%20nanoparticle+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hepsin%20and%20nanoparticle+human)]

No publication is currently available.

## NIH Support

CA86355, CA119349, CA090381, CA92782, AG21404

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
4 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
5 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
6 Wu Q., Parry G. (2007). Hepsin and prostate cancer. Front Biosci.
7 Stephan C., Yousef G.M., Scorilas A., Jung K., Jung M., Kristiansen G., Hauptmann S., Kishi T., Nakamura T., Loening S.A., Diamandis E.P. (2004). Hepsin is highly over expressed in and a new candidate for a prognostic indicator in prostate cancer. J Urol.
8 Klezovitch O., Chevillet J., Mirosevich J., Roberts R.L., Matusik R.J., Vasioukhin V. (2004). Hepsin promotes prostate cancer progression and metastasis. Cancer Cell.
9 Kelly K.A., Setlur S.R., Ross R., Anbazhagan R., Waterman P., Rubin M.A., Weissleder R. (2008). Detection of early prostate cancer using a hepsin-targeted imaging agent. Cancer Res.